# ^111^In-DTPA-Poly(ethylene glycol)-anti-epidermal growth factor receptor antibody C225

Chemical name: | ^111^In-DTPA-Poly(ethylene glycol)-anti-epidermal growth factor receptor antibody C225
Abbreviated name: | ^111^In-DTPA-PEG-C225
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor
Target Category: | Receptor-ligand binding
Method of detection: | SPECT, gamma imaging
Source of signal: | ^111^In
Activation: | Not required
Studies: | - In vitro; - Rodents | Structure of anti-EGFR monoclonal antibody C225 linked to PEG and DTPA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=+C225+imaging&WebEnv=0X1CBGbvevdligXp8RJCH2qgU9NwqYVD6_Kwgd3rDEq0CfGjFoXCogQBemDst4bLh7eu7NF8P5lXZ%40D74F7E8566941A70_0047SID&WebEnvRq=1)]

The epidermal growth factor receptor (EGFR) is a transmembrane glycoprotein that mediates biological activity through an intracellular tyrosine kinase signaling pathway. This receptor is known to be overexpressed in a variety of human malignancies, and the degree of expression often indicates the clinical outcome for the patient (1). Blocking EGFR activity appears to be an effective approach for the treatment of cancers, and a variety of agents, including monoclonal antibodies (MAb), have been developed for this purpose (2). The human-mouse chimeric MAb C225 was developed to target the EGFR and was demonstrated to inhibit the tyrosine kinase signaling pathway of this receptor. C225 was also shown to inhibit the proliferation of tumor cell lines expressing EGFR (3). This MAb is currently being evaluated in several clinical trials for the treatment of human breast, colon, head and neck, lung, prostate, and cervical cancers (4, 5). However, to determine the possible response of a patient, it is necessary to evaluate the degree of EGFR expression in the tumors by immunohistology before and after the MAb treatment. This is an invasive procedure and, because of tumor heterogeneity and metastasis, some tumors may be inaccessible and may be overlooked during patient evaluation (5). Therefore, a radiochemical targeted to the EGFR would be a useful tool to determine the level of EGFR expression in the tumor cells and could help select patients who are most likely to benefit from MAb therapy (5).

Using diethylene triamine pentaacetic acid (DTPA), the radioactive metal chelator indium (^111^In) was linked to C225 and the radiolabeled MAb (^111^In-DTPA-C225) was used in a phase 1 clinical trial to image human squamous cell carcinomas expressing high levels of EGFR (6). As a result of nonspecific uptake of radioactivity, a considerable amount of the radiolabel was detected in the liver of patients undergoing the treatment. A similar observation was made when another MAb against EGFR, MAb 528, was labeled with ^111^In using DTPA. This radiolabeled MAb accumulated in the kidneys as well as the liver (7). These studies indicated a limited usefulness of the two radiolabeled MAbs for the detection of tumors and metastasis in the thorax.

In an attempt to improve the specificity of radiolabeled C225 uptake, Wen et al. (8) synthesized the MAb conjugated to polyethylene glycol (PEG), along with DTPA, to obtain DTPA-PEG-C225. The conjugated MAb was then radiolabeled with ^111^In and evaluated for the detection of xenograft tumors expressing EGFR in nude mice (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA-PEG-C225+synthesis&WebEnv=0mdN_ZwcenT-CCRmSj-kZYxQ4XYo6WTT4WuAJt_Nef-lW9GZhGAGiO8Gn1yJwcLsR4kVVOtRs1bAOi%40D74F38CA66825AD0_0130SID&WebEnvRq=1)]

The synthesis of ^111^In-DTPA-PEG-C225 has been described in detail by Wen et al. (8). Briefly, DTPA-PEG-amine (DTPA-PEG-NH_2_) was prepared by stirring a mixture of DTPA-dianhydride, triethylamine (TEA), and t-Boc-NH-PEG-NH_2_ in chloroform at room temperature for 2 h. After the reaction was complete, the chloroform and TEA were removed under vacuum. The t-Boc protecting group was removed without purification by adding TFA to the resulting residue and stirring at room temperature for 4 h. DTPA-PEG-NH_2_ was purified by dialysis against phosphate-buffered saline (PBS) and deionized water. The product yield of this reaction was 95%.

The purified DTPA-PEG-NH_2_ was reacted with S-acetylthioacetate (SATA) in chloroform for 1 h, purified by dialysis, and passed through a gel filtration column to obtain DTPA-PEG-acetylthioacetate. The yield from this reaction and purification was 92%.

Maleimide-activated C225 was prepared by adding N-γ-maleimidobutyryloxysuccinimide (GMBS) in dimethylformamide (DMF) to an aqueous solution of C225 and stirring the mixture at room temperature for 1 h. The product was purified on a PD-10 column. To obtain DTPA-PEG-SH, which contains free sulfhydral groups, for conjugation with activated C225, the protecting groups on DTPA-PEG-SATA were removed by the addition of hydroxylamine and incubation at room temperature for 30 min. The DTPA-PEG-SH was then mixed with maleimide-activated C225 in a 2:1 molar ratio and the mixture was incubated at 4ºC overnight. Unreacted DTPA-PEG-SH was removed by gel filtration on a Sephacryl S-200 HR column with PBS as the elution buffer.

Four DTPA-PEG-C225 conjugates containing 1:10, 1:20, 1:30, and 1:40 molar ratios of MAb to GMBS were synthesized and the physiochemical properties of these conjugates are detailed by Wen et al. (8). Approximately 20–25% (in the 1:10 ratio conjugate), 40% (in the 1:20 ratio conjugate), 60% (in the 1:30 ratio conjugate), and 70% (in the 1:40 ratio conjugate) of the amino groups in the four conjugates were substituted, respectively.

For radiolabeling, the antibody conjugate was incubated with ^111^InCl_3_ in sodium acetate buffer at room temperature for 15 min. Free ^111^In was removed by gel filtration on a PD-10 column using PBS as the elution buffer. The radiochemical yield was >70% and the purity was >97 to 99%. The authors did not provide specific activity of the labeled MAb in the publication.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA-PEG-C225+in+vitro&WebEnv=0DyxdewZqfMiWl0vV5rITHhcz-HC2rZwgNFF3ARULApDgTSR8Bsstv1SKh4NPkQ43YIzo2XVDASGYe%40D74F38CA66825AD0_0130SID&WebEnvRq=1)]

The binding and biological activity of ^111^In-DTPA-PEG-C225 was evaluated with in vitro assays using cells that express high levels of EGFR (8). Human breast cancer MDA-MB-468 cells were shown to bind increasing radioactivity with increasing concentrations of ^111^In-DTPA-PEG-C225 that plateaued at 2 µg/mL of the labeled antibody. The binding of ^111^In-DTPA-PEG-C225 was observed to be displaced by unlabeled C225 in a dose-dependent manner, indicating that the radiochemical had a specificity for EGFR similar to that of the parent antibody.

The receptor binding affinity of ^111^In-DTPA-PEG-C225 with different degrees of pegylation was investigated using A431 cells. The cells were exposed to the radiochemical MAb conjugated to different amounts of PEG and subsequently lysed (8). The antibody-bound EGFR was immunoprecipitated from the lysates and visualized on a Western blot. It was observed that the amount of EGFR immunoprecipitated by the C225 conjugates (with C225:GMBS molar ratios of 1:10, 1:20, and 1:40, respectively) decreased with an increase in the degree of pegylation, indicating that the PEG modification altered the binding affinity of the antibody.

The biological activity of unlabeled DTPA-PEG-C225 was also assessed with an antiproliferation assay (8). For this, human colon cancer DiFi cells, which undergo apoptosis when the EGFR tyrosine kinase activity is blocked, were exposed to unlabeled DTPA-PEG-C225. It was observed that the modified antibody inhibited DiFi cell proliferation, indicating that the agent induced apoptosis in the cells similar to the C225 antibody.

Pharmacokinetic studies showed that PEG modification of the C225 MAb did not increase the blood circulating half-life of the antibody (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA-PEG-C225+rodentia&WebEnv=0VplvGvA2HNTMIw_zUyW4fG3FkkbfQXhMRJCxX79jSm2PFr9aFLWJD9GDA_hOePEdSHJd8bHZUfwGO%40D74F38CA66825AD0_0130SID&WebEnvRq=1)]

The imaging characteristics of ^111^In-DTPA-PEG-C225 were evaluated in nude mice bearing A431- or EGFR-negative MDA-MB-435 cell tumors or EGFR-positive MDA-MB-468 cell tumors (5). The mice were injected with the 20% and 60% amino-substituted preparations of ^111^In-DTPA-PEG-C225, respectively. The A431 tumor xenografts showed a similar uptake of radioactivity with or without PEG-modified DTPA-C225. The uptake was however reduced by 38–45% in the liver with increased pegylation of the antibody. The A431 and MDA-MB-468 tumors were clearly visible with ^111^In-DTPA-PEG-C225, but the MDA-MB-435 xenografts, which express low levels of EGFR, were not.

The tumor/blood ratios for ^111^In-DTPA-PEG-C225 in the A431 and MDA-MB-468 xenografts were ~three-fold higher than the ratios in the MDA-MB-435 tumors (5). Pretreatment of the mice with unlabeled C225 reduced the radioactivity uptake significantly (by ~60%) in the liver of these animals. In addition, the pretreatment reduced the tumor/blood ratios 2.5- to 2.7-fold in mice bearing the A431 or MDA-MB-468 tumor xenografts. However, no difference was noted in the ratios for the pretreated mice with MDA-MB-435 tumors.

From this study it was concluded that pegylation of C225 significantly reduced the nonspecific antibody uptake by the liver. In addition, ^111^In-DTPA-PEG-C225 was selectively taken up by tumors expressing high levels of EGFR. The study also showed that pegylation is a suitable strategy to link a monoclonal antibody with a metal chelator.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In-DTPA-PEG-C225+Non-Primate+Mammals&WebEnv=0-r3rhAIwWOKEVUZH9y72l7_-jUMerHiBaeHU44p5vELiPyF7wudbsODpn1PS4AKqXtJbsemtkxLL%40D74F7E8566941A70_0047SID&WebEnvRq=1)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In-DTPA-PEG-C225+Non-Human+Primates&WebEnv=0LJqRQ0472pEWIEq3RvSzjvAH6cjH2CL-jXroN_3JTFdZSfysh6iMrrM3Ts_se2mWR0ep_R0cseIj%40D74F7E8566941A70_0047SID&WebEnvRq=1)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In-DTPA-PEG-C225+Human+Studies&WebEnv=0c0y1nDqYFghznxo8cxFPIjjKaesLENtubOWx2aA_Ru1QMB0qbWTrHJUbkJAJLA7J9-GALr_FApfQ%40D74F7E8566941A70_0047SID&WebEnvRq=1)]

No publications are currently available.

## References

1 Lammering G. (2005). Molecular predictor and promising target: will EGFR now become a star in radiotherapy?. Radiother Oncol.
2 Imai K., Takaoka A. (2006). Comparing antibody and small-molecule therapies for cancer. Nat Rev Cancer.
3 Harding J., Burtness B. (2005). Cetuximab: an epidermal growth factor receptor chemeric human-murine monoclonal antibody. Drugs Today (Barc).
4 Herbst R.S. Langer C.J. Epidermal growth factor receptors as a target for cancer treatment: the emerging role of IMC-C225 in the treatment of lung and head and neck cancers Semin Oncol 2002 29 Suppl 4 1 27 36 11894011
5 Wen X., Wu Q.P., Ke S., Ellis L., Charnsangavej C., Delpassand A.S., Wallace S., Li C. (2001). Conjugation with (111)In-DTPA-poly(ethylene glycol) improves imaging of anti-EGF receptor antibody C225. J Nucl Med.
6 Divgi C.R., Welt S., Kris M., Real F.X., Yeh S.D., Gralla R., Merchant B., Schweighart S., Unger M., Larson S.M., et al. (1991). Phase I and imaging trial of indium 111-labeled anti-epidermal growth factor receptor monoclonal antibody 225 in patients with squamous cell lung carcinoma. J Natl Cancer Inst.
7 Reilly R.M., Kiarash R., Sandhu J., Lee Y.W., Cameron R.G., Hendler A., Vallis K., Gariepy J. (2000). A comparison of EGF and MAb 528 labeled with 111In for imaging human breast cancer. J Nucl Med.
8 Wen X., Wu Q.P., Lu Y., Fan Z., Charnsangavej C., Wallace S., Chow D., Li C. (2001). Poly(ethylene glycol)-conjugated anti-EGF receptor antibody C225 with radiometal chelator attached to the termini of polymer chains. Bioconjug Chem.